# anti-1-Amino-2-[^18^F]fluorocyclobutane-1-carboxylic acid

Chemical name: | anti-1-Amino-2-[^18^F]fluorocyclobutane-1-carboxylic acid
Abbreviated name: | anti-2-[^18^F]FACBC
Synonym:
Agent category: | Compound
Target: | L-type amino acid transporter
Target category: | Transporter
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=facbc%5BAll%20Fields%5D)]

A variety of ^11^C- and ^18^F-labeled amino acids have been studied for potential use in positron emission tomography (PET) oncology (1, 2). Most brain tumors show an increased uptake of amino acids as compared with normal brain tissue (3). These amino acids are composed of naturally occurring amino acids, such as L-[^11^C]leucine, L-[^11^C]methionine, and L-[^11^C]tyrosine, and non-natural amino acids, such as [^11^C]aminoisobutyric acid, [^11^C]1-aminocyclopentane-1-carboxylic acid, and [^11^C]1-aminocyclobutane-1-carboxylic acid. ^123^I-Labeled amino acids are also used in imaging in oncology (4-6). The natural amino acids are taken up by tumor cells through an energy-independent L-type amino acid transporter system and retained in tumor cells because of their higher than normal metabolic pathways, including incorporation into proteins (4). L-[^11^C]Methionine and [^18^F]fluorotyrosine have been widely used in the detection of tumors, but are not approved by the FDA. On the other hand, the non-natural amino acids are not metabolized but are taken up through both the L-type transporter and the energy-dependent A-type transporter (7). Therefore, they can accumulate intracellularly in high concentrations. In this chapter, anti-1-Amino-2-[^18^F]fluorocyclobutane-1-carboxylic acid (anti-2-[^18^F]FACBC) was shown to have a high tumor/brain ratio (8). Therefore, anti-2-[^18^F]FACBC could be a useful tracer in PET tumor imaging.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=amino%20acid%20(transporter%20OR%20transporters)+AND+micad%5Bbook%5D)
- Gene information in NCBI (L-type amino acid transporter (http://www.ncbi.nlm.nih.gov/gene/23428), A-type amino acid transporter (http://www.ncbi.nlm.nih.gov/gene/54407))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Amino acid transporters (http://www.ncbi.nlm.nih.gov/omim?Db=omim&Cmd=DetailsSearch&Term=amino%5BAll+Fields%5D+AND+acid%5BAll+Fields%5D+AND+transporter%5BAll+Fields%5D))
- Clinical trials (Amino acid transporters (http://www.clinicaltrials.gov/ct2/results?term=amino+acid+transporters))
- Drug information in FDA (Amino acid transporters (http://google2.fda.gov/search?q=amino+acid+transporters&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=13&y=15))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FACBC+and+synthesis)]

Nucleophilic fluorination of syn-cyclic sulfamidate precursor with K[^18^F]F/Kryptofix2.2.2 and subsequent acidic hydrolysis and purification provided a radiosynthesis yield of 29.5 ± 5.4% (decay-corrected, n = 5) of anti-2-[^18^F]FACBC at the end of synthesis (8). A radiochemical purity of 99% was obtained. The total synthesis time was 85 min. The specific activity of anti-2-[^18^F]FACBC was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FACBC+and+in+vitro)]

Yu et al. (8) showed that anti-2-[^18^F]FACBC entered rat 9L gliosarcoma tumor cells in culture with 3.3 ± 0.1% injected dose (ID)/5 × 10^5^ cells (n = 3) at 30 min of incubation. anti-2-[^18^F]FACBC uptake into rat 9L gliosarcoma tumor cells in culture was reduced by 59%, 33%, and 73% by the presence of 10 mM 2-aminobicyclo[2.2.1]heptane-2-carboxylic acid (L-type transporter inhibitor), N-methyl-α-aminoisobutyric acid (A-type transporter inhibitor), and a mixture of alanine, cysteine, and serine (ACS), respectively. The data suggest that anti-2-[^18^F]FACBC is predominantly transported into 9L cells via both L-type and A-type amino acid transporters. On the other hand, anti-3-[^18^F]FACBC is predominantly an L-type transporter substrate.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FACBC+and+rodentia)]

Ex vivo biodistribution studies of anti-2-[^18^F]FACBC were performed in rats (n = 4/group) implanted intracerebrally with 9L gliosarcoma (8). Accumulation of anti-2-[^18^F]FACBC in the tumors was 0.51, 0.66, 0.65, and 0.60% ID/g at 15, 30, 60, and 120 min after injection, respectively. The accumulation in the contralateral brain tissue was <0.04% ID/g at these time points. The tumor/brain ratios were 12, 17, 14, and 26 at 15, 30, 60, and 120 min, respectively. The accumulation in the heart, muscle, bone, liver, lung, and blood was low. anti-3-[^18^F]FACBC and [^18^F]FDG exhibited tumor/brain ratios of 6.6 and 0.84, respectively, at 60 min in the same tumor model (9). No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FACBC+and+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FACBC+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=facbc%5BAll%20Fields%5D%20AND%20human)]

No publication is currently available.

## References

1 Coleman R.E., Hoffman J.M., Hanson M.W., Sostman H.D., Schold S.C. (1991). Clinical application of PET for the evaluation of brain tumors. J Nucl Med.
2 Kaschten B., Stevenaert A., Sadzot B., Deprez M., Degueldre C., Del Fiore G., Luxen A., Reznik M. (1998). Preoperative evaluation of 54 gliomas by PET with fluorine-18-fluorodeoxyglucose and/or carbon-11-methionine. J Nucl Med.
3 Herholz K., Heiss W.D. (2004). Positron emission tomography in clinical neurology. Mol Imaging Biol.
4 Jager P.L., Vaalburg W., Pruim J., de Vries E.G., Langen K.J., Piers D.A. (2001). Radiolabeled amino acids: basic aspects and clinical applications in oncology. J Nucl Med.
5 Langen K.J., Pauleit D., Coenen H.H. (2002). 3-[(123)I]Iodo-alpha-methyl-L-tyrosine: uptake mechanisms and clinical applications. Nucl Med Biol.
6 Lahoutte T., Caveliers V., Camargo S.M., Franca R., Ramadan T., Veljkovic E., Mertens J., Bossuyt A., Verrey F. (2004). SPECT and PET amino acid tracer influx via system L (h4F2hc-hLAT1) and its transstimulation. J Nucl Med.
7 Palacin M., Estevez R., Bertran J., Zorzano A. (1998). Molecular biology of mammalian plasma membrane amino acid transporters. Physiol Rev.
8 Yu W., Williams L., Camp V.M., Olson J.J., Goodman M.M. (2010). Synthesis and biological evaluation of anti-1-amino-2-[18F]fluoro-cyclobutyl-1-carboxylic acid (anti-2-[18F]FACBC) in rat 9L gliosarcoma. Bioorg Med Chem Lett.
9 Shoup T.M., Olson J., Hoffman J.M., Votaw J., Eshima D., Eshima L., Camp V.M., Stabin M., Votaw D., Goodman M.M. (1999). Synthesis and evaluation of [18F]1-amino-3-fluorocyclobutane-1-carboxylic acid to image brain tumors. J Nucl Med.